# D-Cys-D-Asp-Gly-Tyr(3-NO_2_)-Gly-ProOH-Asn-D-Cys-biotin-streptavidin-Cy5.5

Chemical name: | D-Cys-D-Asp-Gly-Tyr(3-NO_2_)-Gly-ProOH-Asn-D-Cys-biotin-streptavidin-Cy5.5
Abbreviated name: | LXY2-biotin-SA-Cy5.5
Synonym: | cdGT(3-NO_2_)GBNc-biotin-SA-Cy5.5
Agent category: | Peptide
Target: | Integrin α_3_
Target category: | Receptor
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=152013007), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=152013006) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3675) for more information about integrin α_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LXY1)]

Optical fluorescence imaging is increasingly used to obtain biological functions of specific targets small animals (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have a wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging.

Integrins are a family of cell surface heterodimeric glycoproteins that mediate diverse biological events involving cell–cell and cell–matrix interactions (3). They consist of an α and a β subunit, and they are important for cell adhesion and signal transduction. The α_3_β_1_ integrin plays an important role in normal lung, kidney, cerebral cortical, and epithelial development (4). On the other hand, it affects tumor growth, tumor invasiveness, and metastasis, as the α_3_ integrin is strongly expressed on tumor cells (5, 6). D-Cys-D-Asp-Gly-Leu-Gly-ProOH-Asn-D-Cys (LXY1), a cyclic peptide, was identified to bind to α_3_ integrin on human ovarian cancer cells using “one-bead one compound” combinatorial libraries (7, 8). LXY1 was conjugated with Cy5.5 via biotin-streptavidin (SA) to study in vivo biodistribution of the tracer in tumor-bearing mice. LXY1-biotin-SA-Cy5.5 was found to have a high specific accumulation in α_3_-positive human glioblastoma U-87MG cells in nude mice (9). Another LXY1 analog, D-Cys-D-Asp-Gly-Tyr(3-NO_2_)-Gly-ProOH-Asn-D-Cys (LXY2), was identified to exhibit a higher binding affinity than LXY1 (10). LXY2 was conjugated with Cy5.5 via biotin-SA to study in vivo biodistribution of the tracer in tumor-bearing mice. LXY2-biotin-SA-Cy5.5 was found to have a high specific accumulation in α_3_-positve human breast adenocarcinoma MDA-MB-231 cells in nude mice. Cy5.5 is a NIR fluorescence dye with an absorbance maximum at 675 nm and an emission maximum at 694 nm with a high extinction coefficient of 250,000 M^-1^cm^-1^.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LXY1+and+synthesis)]

LXY2 and LXY2-biotin were constructed using solid-phase synthesis (10). SA-Cy5.5 (1.8 nmol) and LXY2-biotin (7.2 nmol) were incubated for 18 h at 4°C to form LXY2-biotin-SA-Cy5.5 (molecular weight, 64 kDa) complexes with a 4:1 molar ratio of biotin/SA.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LXY1+and+in+vitro)]

Xiao et al. (9) showed that the binding affinity (K_d_) of LXY1-biotin for integrin α_3_ on U-87MG cells was 0.5 ± 0.1 µM. The LXY1-biotin binding was completely inhibited by excess LXY1 and anti-α_3_ antibody. Yao et al. (10) showed that LXY1-biotin bound only to integrin α_3_ and not to other integrins tested (α_1_, α_2_, α_3_, α_5_, α_6_, α_9_, α_V_, β_1_, β_2_, β_3_, β_4_, and β_5_) and had a K_d_ value of 0.4 ± 0.1 µM for integrin α_3_ on MDA-MB-231 cells. Using the MDA-MB-231 binding assay, IC_50_ values of LXY1 and LXY2 were 550 ± 0.17 and 57 ± 0.01 nM, respectively. The binding of LXY2-biotin on the MDA-MB-231 cells was inhibited by LXY2 and anti-α_3_ antibody.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LXY1+and+rodentia)]

Biodistribution studies of LXY2-biotin-SA-Cy5.5 were evaluated in nude mice bearing subcutaneous MDA-MB-231 and K562 (α_3_-negatve) xenografts (10). Ex vivo images were obtained after injection of 7.2 nmol LXY1-biotin-SA-Cy5.5 at 6 h after injection. The NIR fluorescence intensities of LXY2-biotin-SA-Cy5.5 in the MDA-MB-231 tumor, liver, and kidneys were high, with low NIR fluorescence intensities in the K562 tumors, skin, intestine, spleen, and muscle. Pretreatment with 0.13 nmol anti-α_3_ integrin antibody 1 h before administration of LXY2-biotin-SA-Cy5.5 showed that accumulation of the imaging probe in the MDA-MB-231 tumor was almost completely blocked by the anti-α3 integrin antibody. On the other hand, the pretreatments had no effect on the NIR fluorescence signals in the liver and kidneys. Whole-body NIR fluorescence imaging showed that the MDA-MB-231 tumor showed a peak NIR fluorescence signal at 6 h and slowly washed out. However, the tumor was still clearly visualized at 72 h.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LXY1+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LXY1+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LXY1+and+human)]

No publication is currently available.

## NIH Support

R01 CA115483, U19 CA113298,

## References

1 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
2 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
3 Hynes R.O., Lively J.C., McCarty J.H., Taverna D., Francis S.E., Hodivala-Dilke K., Xiao Q. (2002). The diverse roles of integrins and their ligands in angiogenesis. Cold Spring Harb Symp Quant Biol.
4 Hynes R.O. (2002). Integrins: bidirectional, allosteric signaling machines. Cell.
5 Albelda S.M., Mette S.A., Elder D.E., Stewart R., Damjanovich L., Herlyn M., Buck C.A. (1990). Integrin distribution in malignant melanoma: association of the beta 3 subunit with tumor progression. Cancer Res.
6 Hynes R.O. (2002). A reevaluation of integrins as regulators of angiogenesis. Nat Med.
7 Aina, O.H., R. Liu, J.L. Sutcliffe, J. Marik, C.X. Pan, and K.S. Lam, From Combinatorial Chemistry to Cancer-Targeting Peptides. Mol Pharm, 2007
8 Aina O.H., Marik J., Liu R., Lau D.H., Lam K.S. (2005). Identification of novel targeting peptides for human ovarian cancer cells using "one-bead one-compound" combinatorial libraries. Mol Cancer Ther.
9 Xiao W., Yao N., Peng L., Liu R., Lam K.S. (2009). Near-infrared optical imaging in glioblastoma xenograft with ligand-targeting alpha3 integrin. Eur J Nucl Med Mol Imaging.
10 Yao N., Xiao W., Wang X., Marik J., Park S.H., Takada Y., Lam K.S. (2009). Discovery of targeting ligands for breast cancer cells using the one-bead one-compound combinatorial method. J Med Chem.